# N(ε)-(3-[^131^I]Iodobenzoyl)-Lys^5^-N(α)-maleimido-Gly^1^-GEEEK-anti-HER2 nanobody 5F7GGC

Chemical name: | N(ε)-(3-[^131^I]Iodobenzoyl)-Lys^5^-N(α)-maleimido-Gly^1^-GEEEK-anti-HER2 nanobody 5F7GGC
Abbreviated name: | [^131^I]IB-Mal-D-GEEEK-Nb
Synonym:
Agent category: | Antibody fragment, nanobody
Target: | Epidermal growth factor receptor (EGFR, HER2)
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^131^I
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4503491), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_001963.2) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1950) for more information about EGF.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=5F7GGC)]

Epidermal growth factor (EGF) is a 53-amino-acid growth factor (6.2 kDa) that is secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF and at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors, including EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2; however, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 and HER2 are overexpressed on many solid tumor cells, such as breast, non–small-cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with a poor patient prognosis because high levels of expression lead to increased cell proliferation (7-10).

Trastuzumab, a humanized immunoglobulin G_1_ (IgG_1_) monoclonal antibody (mAb) against the extracellular domain of recombinant HER2 (11), was labeled with ^111^In (^111^In-trastuzumab (http://www.ncbi.nlm.nih.gov/books/NBK23144/)) (12-14) for use with single-photon emission computed tomography (SPECT) to image EGFR expression on solid tumors. However, the pharmacokinetics of the intact radiolabeled mAb, with high liver uptake and slow blood elimination, are generally not ideal for imaging (15, 16). Smaller antibody fragments, such as scFv, Fab, or F(ab')_2_, have better imaging pharmacokinetics because they are rapidly excreted by the kidneys. Nanobodies are the smallest intact antigen-binding fragments (15 kDa) isolated from heavy-chain camelid antibodies and exhibit efficient and specific tumor targeting (17-19). Anti-HER2 nanobody 5F7GGC was radiolabeled with ^131^I using N(ε)-(3-[^131^I]iodobenzoyl)-Lys^5^-N(α)-maleimido-Gly^1^-GEEEK ([^131^I]IB-Mal-D-GEEEK) to form N(ε)-(3-[^131^I]iodobenzoyl)-Lys^5^-N(α)-maleimido-Gly^1^-GEEEK-anti-HER2 nanobody 5F7GGC ([^131^I]IB-Mal-D-GEEEK-Nb) for use with in vivo SPECT imaging of HER2 expression in tumors in mice (20).

### Related Resource Links:

- Chapters in MICAD (HER2 (http://www.ncbi.nlm.nih.gov/books?term=HER2%20AND%20micad%5Bbook%5D), HER2 nanobody (http://www.ncbi.nlm.nih.gov/books?term=HER2%20nanobody%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (HER2 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2064))
- Articles in Online Mendelian Inheritance in Man (OMIM) (HER2 (http://omim.org/entry/164870))
- Clinical trials (trastuzumab (http://www.clinicaltrials.gov/ct2/results?term=Trastuzumab))
- Drug information in FDA (trastuzumab (http://google2.fda.gov/search?q=Trastuzumab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=14))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=5F7GGC%20and%20synthesis)]

Nanobody 5F7 was produced as a hexahistidine-tagged protein in Escherichia coli. Nanobody 5F7 with a C-terminal cysteine (5F7GGC) was produced in Pichia pastoris (20). A solution of 5F7GGC (6.4 nmol) was treated with 2-iminothiolane (148 nmol) to introduce two sulfhydryl groups per nanobody. The thiol-derivatized 5F7GGC nanobody was labeled with 7.4–59.2 MBq (0.2–1.6 mCi) [^131^I]IB-Mal-D-GEEEK for 45 min at room temperature. [^131^I]IB-Mal-D-GEEEK-Nb was purified with PD-10 column chromatography, with 59.6 ± 9.4% (n = 15) labeling efficiency. The specific activity was 0.22–5.28 MBq/nmol (0.06–0.14 mCi/nmol). [^131^I]IB-Mal-D-GEEEK-Nb was composed of 69.0 ± 5.7% monomer and 31.0 ± 5.7% dimer.

For comparison studies, 5F7GGC (6.4 nmol) was labeled with 11.1–92.5 MBq (0.3–2.5 mCi) Na[^125^I]iodide using the Iodogen method (20). ^125^I-Nb was purified with PD-10 column chromatography, with 83.6 ± 5.0% (n = 10) labeling efficiency. The specific activity was 0.55–13.64 MBq/nmol (0.015–0.37 mCi/nmol). ^125^I-Nb was composed of 63.4 ± 0.6% monomer and 36.6 ± 0.6% dimer.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=5F7GGC%20and%20in%20vitro)]

In vitro saturation binding assays of [^131^I]IB-Mal-D-GEEEK-Nb and ^125^I-Nb to BT474M1 human breast carcinoma cells expressing HER2 receptor were performed. There was a single class of high-affinity binding sites, with K_d_ values of 3.2 ± 1.0 nM and 1.8 ± 0.6 nM for [^131^I]IB-Mal-D-GEEEK-Nb and ^125^I-Nb, respectively. The immunoreactivity values were 75.3 ± 19.6% and 60.5 ± 4.2% for [^131^I]IB-Mal-D-GEEEK-Nb and ^125^I-Nb, respectively. Cellular internalization of [^131^I]IB-Mal-D-GEEEK-Nb was 56.9% at 1 h and 58.3% at 24 h. Cellular internalization of ^125^I-Nb was 61.4% at 1 h and 32.4% at 24 h.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=5F7GGC%20and%20rodentia)]

Pruszynski et al. (20) performed ex vivo biodistribution studies of 0.15 MBq (4 µCi) [^131^I]IB-Mal-D-GEEEK-Nb (26 pmol) or ^125^I-Nb (13 pmol) in nude mice (n = 5/group) bearing BT474M1 xenografts at 1, 2, 4, 8, and 24 h after injection. Tumor accumulation (percent of injected dose/g (% ID/g)) of [^131^I]IB-Mal-D-GEEEK-Nb (4.7 ± 0.6% ID/g at 8 h and 3.6 ± 1.2% at 24 h) was higher than that of ^125^I-Nb (2.9 ± 0.2% ID/g at 8 h and 1.2 ± 0.3% at 24 h) at all time points (P < 0.05). For [^131^I]IB-Mal-D-GEEEK-Nb, the highest radioactivity accumulation at 2 h was observed in the kidneys (179% ID/g), followed by the liver (5.2% ID/g), tumor (4.4% ID/g), lung (2.0% ID/g), spleen (1.3% ID/g), blood (0.9% ID/g), small intestine (0.6% ID/g), bone (0.6% ID/g), heart (0.5% ID/g), stomach (0.4% ID/g), muscle (0.2% ID/g), and thyroid (0.03% ID/organ). ^125^I-Nb exhibited higher accumulation in most of the normal tissues except the kidneys (12.1% ID/g). The thyroid and stomach accumulation of [^131^I]IB-Mal-D-GEEEK-Nb was 40- to 50-fold lower than that of ^125^I-Nb, suggesting that [^131^I]IB-Mal-D-GEEEK-Nb is less susceptible to deiodination than ^125^I-Nb. The tumor/blood and tumor/muscle ratios for [^131^I]IB-Mal-D-GEEEK-Nb were significantly higher than those for ^125^I-Nb at all time points (P < 0.05). Administration of 1,500-fold molar excess trastuzumab 24 h before the tracers decreased the 2-h tumor accumulation of [^131^I]IB-Mal-D-GEEEK-Nb and ^125^I-Nb by 80% and 67%, respectively. Little inhibition was observed in most of the normal tissues.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=5F7GGC%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=5F7GGC%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=5F7GGC%20and%20human)]

No publication is currently available.

## NIH Support

CA42324, CA154291, CA14236

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer: signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
12 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.
13 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
14 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
15 Olafsen T., Wu A.M. (2010). Antibody vectors for imaging. Semin Nucl Med.
16 Wu A.M. (2009). Antibodies and antimatter: the resurgence of immuno-PET. J Nucl Med.
17 Arbabi Ghahroudi M., Desmyter A., Wyns L., Hamers R., Muyldermans S. (1997). Selection and identification of single domain antibody fragments from camel heavy-chain antibodies. FEBS Lett.
18 Desmyter A., Decanniere K., Muyldermans S., Wyns L. (2001). Antigen specificity and high affinity binding provided by one single loop of a camel single-domain antibody. J Biol Chem.
19 Muyldermans S. (2001). Single domain camel antibodies: current status. J Biotechnol.
20 Pruszynski M., Koumarianou E., Vaidyanathan G., Revets H., Devoogdt N., Lahoutte T., Zalutsky M.R. (2013). Targeting breast carcinoma with radioiodinated anti-HER2 Nanobody. Nucl Med Biol.